# 7-[ ^11^C]Methoxy-1-methyl-9H-[3,4-b]indole

Chemical name: | 7-[^11^C]Methoxy-1-methyl-9H-[3,4-b]indole
Abbreviated name: | [^11^C]HAR
Synonym: | [^11^C]Harmine
Agent category: | Compound
Target: | Monoamine oxidase A (MAO-A)
Target category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Harmine)]

Monoamine oxidase (MAO) is a mitochondrial enzyme which inactivates dopamine, noradrenaline and serotonin in the brain (1, 2). Two isoforms (A and B) of the enzyme have been identified. MAO-A preferentially oxidizes serotonin and noradrenaline, whereas MAO-B preferentially oxidizes phenethylamine. Dopamine is a substrate for both enzymes. MAO-A is predominately associated with depression and anxiety disorders while MAO-B is predominately associated with neurodegenerative disease, such as Parkinson’s disease (PD) as indicated by studies with specific MAO isoform inhibitors (3-5).

For measurements of MAO-A activity, MAO-A inhibitor harmine (HAR) was radiolabeled as [^11^C]HAR for use in positron emission tomography (PET). HAR is a carboline analog, which is a competitive and reversible inhibitor of MAO-A with a K_i_ of 5 nM (6). [^11^C]HAR is being developed as a PET agent for the non-invasive study of brain MAO-A distribution and concentration in patients with psychiatric and neurologic disorders as well as neuroendocrine tumors.

### Related Resource Links:

- Chapters in MICAD (MAO-A (http://www.ncbi.nlm.nih.gov/books?term=MAO-A%20AND%20micad%5Bbook%5D), MAO-B (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=MAO-B+AND+micad%5Bbook%5D))
- Gene information in NCBI (MAO-A (http://www.ncbi.nlm.nih.gov/gene/4128), MAO-B (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=4129))
- Articles in Online Mendelian Inheritance in Man (OMIM) (MAO-A (http://www.ncbi.nlm.nih.gov/omim/309850), MAO-B (http://omim.org/entry/309860))
- Clinical trials (MAO-A (http://www.clinicaltrials.gov/ct2/results?term=MAO-A), MAO-B (http://www.clinicaltrials.gov/ct2/results?term=MAO-B))
- Drug information in FDA (MAO-A (http://google2.fda.gov/search?q=MAO-A&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*), MAO-B (http://google2.fda.gov/search?q=MAO-B&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Harmine%20and%20synthesis)]

Bergstrom et al. (7) reported synthesis of [^11^C]HAR by direct O-methylation of 7-hydroxy-1-methyl-9H-[3,4-b]indole with [^11^C]methyl iodide in the presence of sodium hydroxide in DMSO, with a radiochemical yield of 72.5 ± 3.6% (end of synthesis) after high-performance liquid chromatography purification. Radiochemical purities were >98% with a specific activity of 18-93 GBq/μmol (0.5-2.5 Ci/μmol) and a total synthesis time of 43 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Harmine%20and%20in%20vitro)]

Bergstrom et al. (8) reported that [^11^C]HAR bound rapidly to frozen sections of rat brain with a K_d_ of 2.0 ± 0.7 nM. The binding was reversible by washings. There were about 14-22% non-specific binding, which could not be displaced by 1 µM of HAR. The specific binding was inhibited by various MAO-A inhibitors, such as clorgyline (IC_50_ = 16 nM), esuprone (IC_50_ = 19 nM), and brofaromine (IC_50_ = 50 nM). On the other hand, MAO-B inhibitors (deprenyl and pargyline) were inhibitory only at >1 μM concentrations.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Harmine%20and%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Harmine%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

Jensen et al. (9) reported on PET studies in five adult female Gottingen minipigs with [^11^C]HAR under baseline conditions and after pargyline (a 20-fold more potent inhibitor of MAO-B than of MAO-A). Distribution volumes (DVs) of [^11^C]HAR relative to the arterial input were estimated from parametric images of brain regions of interest. The medial hypothalamus (139 ml/g) and ventral forebrain (139 ml/g) had the highest [^11^C]HAR binding, followed by the thalamus (135 ml/g), locus coeruleus (133 ml/g), striatum (104 ml/g), pituitary (92 ml/g), frontal cortex (91 ml/g), occipital cortex (84 ml/g), and cerebellum (74 ml/g). Pargyline pretreatment (6 mg/kg) reduced the magnitude of DV globally to 34-54 ml/g. Nearly complete inhibition of [^11^C]HAR binding was detected in the occipital cortex, frontal cortex, and striatum, but there was 15-35% of [^11^C]HAR binding resistant to pargyline inhibition in the pituitary gland and diencephalon.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Harmine%20and%20%28primate%20not%20human%29)]

Bergstrom et al. (7, 8) performed [^11^C]HAR PET studies in rhesus monkeys and found rapid accumulation in the brain within minutes after injection. The accumulation of [^11^C]HAR showed high radioactivity in all gray matter regions homogeneously, with a standard uptake value (SUV) of 2.5 at 3.5 min and a final value of 3.7 at 60 min. Pretreatments with various MAO-A inhibitors decreased the SUV to 2.3 at 60 min. Patlak graphic analysis estimated an IC_50_ value of 0.05-0.1 mg/kg for blocking of [^11^C]HAR uptake by HAR in the brain.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Harmine%20and%20human)]

Bergstrom et al. (10) studied 16 healthy male volunteers with [^11^C]HAR PET before and after pretreatment with esuprone (n = 8), moclobemide (n = 4) and placebo (n = 4). The subject was given 200-300 MBq (5.4-9.1 mCi) of [^11^C]HAR with plasma metabolite samplings. The accumulation of [^11^C]HAR in the brain was high in all grey matter regions, with minor differences between different regions of the brain. Patlak graphic analyses revealed an 80% inhibition of [^11^C]HAR binding in the grey matter regions by esurprone and moclobemide. Later, Ginovart et al. (11) confirmed the moclobemide inhibition using a two-tissue compartment model to estimate DV values in regions of interest in the brain. [^11^C]HAR uptake was highest in the thalamus, followed by the temporal cortex=cingulated, occipital cortex, frontal cortex=putamen, and cerebellum. The estimated DV values were highly stable and not different from those estimated with the Logan analyses. There was a 64-79% reduction of [^11^C]HAR binding in the brain after dosing with moclobemide (300 mg daily for 10 days). The fraction of unchanged [^11^C]HAR in the plasma was 90% at 5 min, 46% at 20 min, and 34% at 30 min.

Orlefors et al. (12) showed [^11^C]HAR PET could visualize tumors in 11 patients with midgut carcinoids (MGC) and endocrine pancreatic tumors (EPT). The mean SUV for MGC (n = 4) at 5 min was 7.5 ± 3.9 and for EPT (n = 7) 12.9 ± 2.7, whereas the SUV for normal liver, intestine and pancreas were 3.1 ± 0.5, 3.4 ± 1.2 and 8.9 ± 3.0, respectively.

## References

1 Richards J.G., Saura J., Ulrich J., Da Prada M. (1992). Molecular neuroanatomy of monoamine oxidases in human brainstem. Psychopharmacology (Berl).
2 Saura J., Kettler R., Da Prada M., Richards J.G. (1992). Quantitative enzyme radioautography with 3H-Ro 41-1049 and 3H-Ro 19-6327 in vitro: localization and abundance of MAO-A and MAO-B in rat CNS, peripheral organs, and human brain. J Neurosci.
3 Murphy D.L., Wyatt R.J. (1972). Reduced monoamine oxidase activity in blood platelets from schizophrenic patients. Nature.
4 Murphy D.L., Weiss R. (1972). Reduced monoamine oxidase activity in blood platelets from bipolar depressed patients. Am J Psychiatry.
5 Jarman J., Glover V., Sandler M., Turjanski N., Stern G. (1993). Platelet monoamine oxidase B activity in Parkinson's disease: a re-evaluation. J Neural Transm Park Dis Dement Sect.
6 Kim H., Sablin S.O., Ramsay R.R. (1997). Inhibition of monoamine oxidase A by beta-carboline derivatives. Arch Biochem Biophys.
7 Bergstrom M., Westerberg G., Kihlberg T., Langstrom B. (1997). Synthesis of some 11C-labelled MAO-A inhibitors and their in vivo uptake kinetics in rhesus monkey brain. Nucl Med Biol.
8 Bergstrom M., Westerberg G., Langstrom B. (1997). 11C-harmine as a tracer for monoamine oxidase A (MAO-A): in vitro and in vivo studies. Nucl Med Biol.
9 Jensen S.B., Olsen A.K., Pedersen K., Cumming P. (2006). Effect of monoamine oxidase inhibition on amphetamine-evoked changes in dopamine receptor availability in the living pig: a dual tracer PET study with [11C]harmine and [11C]raclopride. Synapse.
10 Bergstrom M., Westerberg G., Nemeth G., Traut M., Gross G., Greger G., Muller-Peltzer H., Safer A., Eckernas S.A., Grahner A., Langstrom B. (1997). MAO-A inhibition in brain after dosing with esuprone, moclobemide and placebo in healthy volunteers: in vivo studies with positron emission tomography. Eur J Clin Pharmacol.
11 Ginovart N., Meyer J.H., Boovariwala A., Hussey D., Rabiner E.A., Houle S., Wilson A.A. (2006). Positron emission tomography quantification of [11C]-harmine binding to monoamine oxidase-A in the human brain. J Cereb Blood Flow Metab.
12 Orlefors H., Sundin A., Fasth K.J., Oberg K., Langstrom B., Eriksson B., Bergstrom M. (2003). Demonstration of high monoaminoxidase-A levels in neuroendocrine gastroenteropancreatic tumors in vitro and in vivo-tumor visualization using positron emission tomography with 11C-harmine. Nucl Med Biol.